# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-E{E[c(RGDfK)]_2_}_2_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid- E{E[c(RGDfK)]_2_}_2_
Abbreviated name: | ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_
Synonym: | ^64^Cu-Tetrameric RGD peptide
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/ contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29)]

^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-E{E[c(RGDfK)_2_}_2_ (^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_) is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) imaging of tumor vasculature, tumor angiogenesis and osteoclasts (1). ^64^Cu is a positron emitter with a half-life (t_½_) of 12.7 h

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5).These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7).

Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). It has been hypothesized that cyclic RGD peptide may have a faster rate of receptor binding or a slower rate of dissociation from the integrin α_v_β_3_ than linear single-RGD peptides (1). Chen et al. (9) evaluated a cyclic RGD peptide [c(RGDyK)] labeled with ^64^Cu or ^18^F in nude mice bearing breast tumor. They used DOTA for c(RGDyK) conjugation with ^64^Cu. ^64^Cu-DOTA-c(RGDyK) showed prolonged tumor radioactivity retention but persistent liver radioactivity. Wu et al. (1) suggested that a multimeric RGD peptide with more than two repeating cyclic RGD units would further enhance the affinity of the receptor−ligand interactions through the phenomenon of a polyvalency effect. They also suggested that the increase in molecular size might also prolong circulation time and reduce tumor washout rate as well. Consequently, Wu et al. (1) developed a tetrameric RGD peptide, ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_, and they showed that this PET radioligand appeared to have high integrin avidity and favorable biokinetics in nude mice bearing human glioma.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20synthesis)]

Wu et al. (1) reported the synthesis of ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_. DOTA-E{E[c(RGDfK)]_2_}_2_ was synthesized through an active ester method by coupling Boc-Glu(OSu)-OSu with E[c(RGDfK)]_2_ followed by deprotection. The monomeric cyclic peptide c(RGDfK) was first prepared via solution cyclization of fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by trifluoroacetic acid (TFA) deprotection in the presence of the free-radical scavenger triisopropylsilane (10). The RGD dimer was then prepared by mixing c(RGDfK) with the Boc-protected glutamic acid activated ester Boc-Glu(OSu)_2_ in triethylamine and stirring at room temperature overnight (10, 11). This yielded Boc-E[c(RGDfK)]_2._ The Boc-group was then removed by dissolving in anhydrous trifluoroacetic acid (TFA) and stirring at room temperature for 5 min. Similarly, the tetramer was prepared by mixing E[c(RGDfK)]_2_ with Boc-E(OSu)_2_ at room temperature (pH 8.5−9.0) overnight and removing the Boc-group by treatment with TFA. E{E[c(RGDfK)]_2_}_2_ was purified by high-performance liquid chromatography (HPLC) (1). DOTA-E{E[c(RGDfK)]_2_}_2_ was synthesized by first activating DOTA with 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) at pH 5.5 for 30 min to produce DOTA-OSSu. DOTA-OSSu was then cooled to 4ºC and reacted with E[c(RGDfK)_2_}_2_. The reaction mixture was adjusted to pH 8.5 and incubated overnight. The DOTA-peptide was purified by high-performance liquid chromatography (HPLC).The overall yield was 25% starting from Boc-Glu. ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_ was prepared by adding ^64^Cu chloride in sodium acetate to DOTA-E{E[c(RGDfK)_2_}_2_ and incubated for 1 h at 50ºC. The final radiolabeled peptide was purified by semipreparative HPLC. The radiochemical purity was >95% and the specific activity was 37 MBq/nmol (1 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20in%20vitro)]

The octanol-water partition coefficient (log P) of ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_ was determined to be −1.60 ± 0.10 in phosphate-buffered saline (pH 7.4) and octanol at room temperature (1).

Wu et al. (1) conducted an in vitro cell integrin receptor-binding assay of unlabeled DOTA-E{E[c(RGDfK)]_2_}_2_ by using ^125^I-echistatin as the integrin-specific radioligand and integrin α_v_β_3_ −positive human glioblastoma U87MG cells. The cell-binding assay demonstrated that DOTA had minimal effect on the receptor avidity. The RGD tetramer had about 3-fold and 10-fold higher integrin avidity than the corresponding dimeric and monomeric RGDs. The inhibition concentration (IC_50_) values (n = 3) for DOTA-E{E[c(RGDfK)]_2_}_2_ and DOTA-E[c(RGDfK)]_2_ were 16.6 ± 1.3 and 48.4 ± 2.8, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20rodentia)]

Biodistribution studies of ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_ were conducted in nude mice bearing human U87MG glioma (1). Each mouse received an i.v. dose of 0.74−1.11 MBq (20−30 μCi) ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_. Rapid blood clearance and high tumor radioactivity accumulation were observed. The tumor radioactivity levels (n = 3) in percent injected dose per g (% ID/g) for the tumor were 9.93 ± 1.05 (0.5 h), 7.61 ± 0.68 (2 h), and 4.56 ± 0.51 (24 h). The tumor/nontarget tissue ratios at 2 h were 34.8 ± 2.7 (tumor/blood), 15.9 ± 1.2 (tumor/muscle), 3.95 ± 0.30 (tumor/intestine), 2.32 ± 0.18 (tumor/liver), and 1.54 ± 0.12 (tumor/kidney). The biologic retention t_½_ of the radioactivity in the tumor was 4.3 h. The tumor radioactivity accumulation of the tetramer appeared to be >2-fold higher than the dimer. The biological t_½_ of ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_ radioactivity in the blood was 0.56 h. In comparison, the biological t_½_ of the dimer radioactivity in the blood was 0.20 h. The kidneys and liver had relatively higher radioactivity levels than other major organs. The kidney radioactivity levels (% ID/g) were 9.02 ± 0.56 (0.5 h) and 2.83 ± 0.22 (24 h). The biological retention t_½_ of the radioactivity was 1.72 h. The liver radioactivity levels (% ID/g) were 4.38 ± 0.39 (1 h) and 2.34 ± 0.18 (24 h). A coinjection dose of 10 mg/kg c(RGDyK) significantly decreased the radioactivity in all tissues except the blood and kidney. The radioactivity level of the tumor was decreased from 9.70% ID/g to 1.75% ID/g.

MicroPET imaging of nude mice bearing U87MG tumor (n = 3) injected with 9.1 MBq (0.245 mCi) ^64^Cu-DOTA-E{E[c(RGDfK)_2_}_2_ clearly visualized the tumor with high tumor-to-contralateral (~5) background contrast up to 18 h after injection (1). A coinjection dose of 10 mg/kg c(RGDyK) decreased the tumor-to-background contrast from 8.7 ± 1.5 to 2.3 ± 0.6.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20human)]

Wu et al. (1) estimated the radiation-absorbed doses of ^64^Cu-DOTA-E{E[c(RGDfK)]_2_}_2_ in the adult human on the basis of the average biodistribution data in nude mice bearing U87MG tumor. The urinary bladder wall appeared to be the critical organ with 0.262 ± 0.0472 mGy/MBq (0.969 ± 0.175 rad/mCi). The total body dose was 0.00235 ± 0.000376 mGy/MBq (0.00869 ± 0.00139 rad/mCi). The estimated doses to the kidneys and liver were 0.0296 ± 0.00184 mGy/MBq (0.110 ± 0.00684 rad/mCi) and 0.0243 ± 0.00156 mGy/MBq (0.0898 ± 0.00576 rad/mCi), respectively.

## NIH Support

NIH NIBIB R21 EB001785, NCI CA93862, NCI R24 CA86307.

## References

1 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
10 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
11 Liu S., Hsieh W.Y., Kim Y.S., Mohammed S.I. (2005). Effect of coligands on biodistribution characteristics of ternary ligand 99mTc complexes of a HYNIC-conjugated cyclic RGDfK dimer. Bioconjug Chem.